# (R)-(-)-2-Chloro-N-[1-^11^C-propyl]n-propylnorapomorphine

Chemical name: | (R)-(-)-2-Chloro-N-[1-^11^C-propyl]n-propylnorapomorphine
Abbreviated name: | 2-Cl-[^11^C]-(-)-NPA
Synonym:
Agent category: | Compound
Target: | D_3_ dopamine receptors
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (1, 2). Dopamine receptors are involved in the pathophysiology of neuropsychiatric diseases, such as Parkinson’s disease, Alzheimer's disease, Huntington’s disease, and schizophrenia (3). Five subtypes of dopamine receptors, D_1_ through D_5_, have been well characterized pharmacologically and biochemically (4). These five subtypes are classified into two subfamilies: D_1_-like (D_1_ and D_5_) and D_2_-like (D_2_, D_3_, and D_4_) dopamine receptors. D_1_-Like and D_2_-like receptors exert synergistic as well as opposite effects at both the biochemical and overall system levels. A great majority of striatal D_1_ and D_2_ receptors are localized postsynaptically on caudate-putamen neurons and to a lesser extent presynaptically on nigrostriatal axons.

Dopamine receptors are G-protein–coupled receptors and exist in high- and low-affinity states with respect to agonist binding. The two states are interconvertible. The high-affinity state is coupled to G-proteins, whereas the low-affinity state is not. Dopamine has a dissociation constant (K_d_) of 7 nM for the high-affinity state (K_high_) and a K_d_ of 1,720 nM for the low-affinity state (K_low_) (5). Under physiological conditions, dopamine is expected to bind predominantly to the high-affinity state, which is ~50% occupied by 10 nM dopamine. The high-affinity state was suggested to be the functional form of the dopamine receptors.

Substituted benzamides, such as sulpiride, raclopride, and iodobenzamide, are specific ligands with only moderate affinity for the D_2_-like receptors, making studies of extrastriatal D_2_ receptors difficult (6-8). In binding studies, ^123^I-labeled epidepride, an analog of isoremoxipride, was found to have high potency and low nonspecific binding, and to be selective for striatal and extrastriatal D_2_ receptors (9). Epidepride has marginal binding to D_4_ receptors, with little affinity for other known neurotransmitter receptors. (S)-N-((1-Allyl-2-pyrrolidinyl)methyl)-5-(3-[^18^F]fluoropropyl)-2,3-dimethoxybenzamide ([^18^F]fallypride), an analog of epidepride, was found to be a selective, high-affinity antagonist of D_2/3_ receptors (10) in positron emission tomography (PET) in vivo studies (11-13). [^18^F]fallypride identified extrastriatal D_2/3_ receptors. However, none of these antagonists distinguish between the high- and low-affinity states of the D_2_ receptors. (-)-N-Propyl-norapomorphine (NPA) was reported to have K_high_ and K_low_ values of 0.07–0.4 and 20–200 nM, respectively (5, 14-16). This provides a >50-fold selectivity for the high-affinity over the low-affinity receptors. NPA has good affinity (K_i_, 0.3 nM) for D_3_ receptors but not other neurotransmitters (17). [^11^C]NPA is being developed as a PET agent for the noninvasive study of the high-affinity state of the D_2_ receptors in the brain. (R)-(-)-2-Chloro-N-[1-^11^C-propyl]n-propylnorapomorphine (2-Cl-[^11^C]-(-)-NPA) has been evaluated as a D_3_-selective probe because 2-Cl-(-)-NPA showed a higher selectivity for D_3_ than for D_2_ (D_3_/D_2_, 3.85) than did (-)-NPA (D_3_/D_2_, 1.75) (18).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=dopamine%20(receptors%20OR%20receptor)+%20AND+Table+AND+micad%5Bbook%5D)
- Gene information in NCBI (D_2_ receptor, (http://www.ncbi.nlm.nih.gov/gene/1813) D_3_ receptor (http://www.ncbi.nlm.nih.gov/gene/1814))
- Articles in OMIM (D_2_ receptor (http://www.ncbi.nlm.nih.gov/omim/126450), D_3_ receptor (http://www.ncbi.nlm.nih.gov/omim/126451))
- Clinical trials (Dopamine receptors (http://www.clinicaltrials.gov/ct2/results?term=dopamine+receptor))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29%20and%20synthesis)]

Palner et al. (18) reported a one-pot synthesis of 2-Cl-[^11^C]-(-)-NPA by reacting [^11^C]propionyl chloride with (-)-chloronorapomorphine hydrobromide and a LiAlH_4_ reduction, with a radiochemical yield of ~9% (based on [^11^C]CO_2_, end of bombardment) and specific activities of 28–45 GBq/μmol (757–1,220 mCi/μmol) at the end of synthesis after C-18 Sep-Pak and purification with high-performance liquid chromatography. Radiochemical purities were >97%. [^11^C]Propionyl chloride was prepared by reacting [^11^C]CO_2_ with ethylmagnesium bromide, followed by reaction with phthaloyl chloride. The total synthesis time was ~40 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29%20and%20in%20vitro)]

In binding to dopamine receptors in membranes of porcine anterior pituitary, [^3^H]NPA had an average K_d_ of 0.26 ± 0.01 nM and a B_max_ of 2.3 ± 0.1 pmol/g tissue (19). 2-Cl-[^11^C]-(-)-NPA exhibited K_i_ values of 4.52 ± 0.98 and 17.26 ± 2.88 nM for D_2_ and D_3_, respectively (18). [^11^C]-(-)-NPA had K_i_ values of 0.12 ± 0.04 and 0.21 ± 0.09 nM for D_2_ and D_3_, respectively. The cLog D values were calculated to be 2.25 and 0.79 for 2-Cl-[^11^C]-(-)-NPA and [^11^C]-(-)-NPA, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29%20and%20rodentia)]

Palner et al. (18) performed ex vivo brain biodistribution studies of 37 MBq (1 mCi) 2-Cl-[^11^C]-(-)-NPA in rats. 2-Cl-[^11^C]-(-)-NPA accumulated more slowly in the striatum than did [^11^C]-(-)-NPA, reaching maximum concentrations after 30 min. The maximal striatal uptake of 2-Cl-[^11^C]-(-)-NPA (standard uptake value (SUV) = 0.72 ± 0.24) was approximately half that of [^11^C]-(-)-NPA (SUV = 1.37 ± 0.18). Nonspecific uptake was similar for the two tracers in the cerebellum (SUV = 0.32–0.33). The striatum/cerebellum ratios were 1.18 and 3.31 for 2-Cl-[^11^C]-(-)-NPA and [^11^C]-(-)-NPA, respectively, at 60 min after injection. 2-Cl-[^11^C]-(-)-NPA was metabolized quickly to one major and two minor less lipophilic metabolites, leaving only 17% of 2-Cl-[^11^C]-(-)-NPA in the plasma after 30 min. The specific binding of 2-Cl-[^11^C]-(-)-NPA was completely blocked by pretreatment with haloperidol (5 mg/kg, 30 min). The authors concluded that 2-Cl-[^11^C]-(-)-NPA is less likely to be more useful as a PET agent than [^11^C]-(-)-NPA because of slower brain uptake and a lower striatum/cerebellum ratio.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29%20and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29%20and%20%28primate%20not%20human%29)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20%28NPA%20or%20propyl-norapomorphine%29%20and%20human)]

No publications are currently available.

## NIH Support

N01MH32004

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Seeman P., Bzowej N.H., Guan H.C., Bergeron C., Reynolds G.P., Bird E.D., Riederer P., Jellinger K., Tourtellotte W.W. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
4 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
5 George S.R., Watanabe M., Di Paolo T., Falardeau P., Labrie F., Seeman P. (1985). The functional state of the dopamine receptor in the anterior pituitary is in the high affinity form. Endocrinology.
6 Gehlert D.R., Wamsley J.K. (1984). Autoradiographic localization of [3H]sulpiride binding sites in the rat brain. Eur J Pharmacol.
7 Lidow M.S., Goldman-Rakic P.S., Rakic P., Innis R.B. (1989). Dopamine D2 receptors in the cerebral cortex: distribution and pharmacological characterization with [3H]raclopride. Proc Natl Acad Sci U S A.
8 Brucke T., Tsai Y.F., McLellan C., Singhanyom W., Kung H.F., Cohen R.M., Chiueh C.C. (1988). In vitro binding properties and autoradiographic imaging of 3-iodobenzamide ([125I]-IBZM): a potential imaging ligand for D-2 dopamine receptors in SPECT. Life Sci.
9 Kessler R.M., Ansari M.S., Schmidt D.E., de Paulis T., Clanton J.A., Innis R., al-Tikriti M., Manning R.G., Gillespie D. (1991). High affinity dopamine D2 receptor radioligands. 2. [125I]epidepride, a potent and specific radioligand for the characterization of striatal and extrastriatal dopamine D2 receptors. Life Sci.
10 Mukherjee J., Yang Z.Y., Das M.K., Brown T. (1995). Fluorinated benzamide neuroleptics--III. Development of (S)-N-[(1-allyl-2-pyrrolidinyl)methyl]-5-(3-[18F]fluoropropyl)-2, 3-dimethoxybenzamide as an improved dopamine D-2 receptor tracer. Nucl Med Biol.
11 Grunder, G., C. Landvogt, I. Vernaleken, H.G. Buchholz, J. Ondracek, T. Siessmeier, S. Hartter, M. Schreckenberger, P. Stoeter, C. Hiemke, F. Rosch, D.F. Wong, and P. Bartenstein, The Striatal and Extrastriatal D2/D3 Receptor-Binding Profile of Clozapine in Patients with Schizophrenia. Neuropsychopharmacology, 2005
12 Mukherjee J., Christian B.T., Narayanan T.K., Shi B., Collins D. (2005). Measurement of d-amphetamine-induced effects on the binding of dopamine D-2/D-3 receptor radioligand, 18F-fallypride in extrastriatal brain regions in non-human primates using PET. Brain Res.
13 Riccardi, P., R. Li, M.S. Ansari, D. Zald, S. Park, B. Dawant, S. Anderson, M. Doop, N. Woodward, E. Schoenberg, D. Schmidt, R. Baldwin, and R. Kessler, Amphetamine-Induced Displacement of [(18)F] Fallypride in Striatum and Extrastriatal Regions in Humans. Neuropsychopharmacology, 2005
14 Gardner B., Strange P.G. (1998). Agonist action at D2(long) dopamine receptors: ligand binding and functional assays. Br J Pharmacol.
15 Lahti R.A., Mutin A., Cochrane E.V., Tepper P.G., Dijkstra D., Wikstrom H., Tamminga C.A. (1996). Affinities and intrinsic activities of dopamine receptor agonists for the hD21 and hD4.4 receptors. Eur J Pharmacol.
16 Seeman P., Watanabe M., Grigoriadis D., Tedesco J.L., George S.R., Svensson U., Nilsson J.L., Neumeyer J.L. (1985). Dopamine D2 receptor binding sites for agonists. A tetrahedral model. Mol Pharmacol.
17 Neumeyer J.L., Neustadt B.R., Oh K.H., Weinhardt K.K., Boyce C.B., Rosenberg F.J., Teiger D.G. (1973). Aporphines. 8. Total synthesis and pharmacological evaluation of (plus or minus)-apomorphine, (plus or minus)-apocodeine, (plus or minus)-N-n-propylnorapomorphine, and (plus or minus)-N-n-propylnorapocodeine. J Med Chem.
18 Palner M., McCormick P., Gillings N., Begtrup M., Wilson A.A., Knudsen G.M. (2010). Radiosynthesis and ex vivo evaluation of (R)-(-)-2-chloro-N-[1-11C-propyl]n-propylnorapomorphine. Nucl Med Biol.
19 Sibley D.R., De Lean A., Creese I. (1982). Anterior pituitary dopamine receptors. Demonstration of interconvertible high and low affinity states of the D-2 dopamine receptor. J Biol Chem.